# N-[2-(3-cyanophenyl)-3-(4-(2-[^18^F]fluorethoxy)phenyl)-1-methylpropyl]-2-(5-methyl-2-pyridyloxy)-2-methylproponamide

Chemical name: | N-[2-(3-cyanophenyl)-3-(4-(2-[^18^F]fluorethoxy)phenyl)-1-methylpropyl]-2-(5-methyl-2-pyridyloxy)-2-methylproponamide
Abbreviated name: | [^18^F]MK-9470
Synonym:
Agent Category: | Compound
Target: | Cannabinoid CB1 receptor
Target Category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of Signal/Contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cannabinoid+CB1+receptor)]

Psychoactive cannabinoids derived from the marijuana plant (Cannabis sativa) have two known types of G-protein–coupled receptors that are linked to adenylate cyclase activity. The cannabinoid-1 receptor (CB1R) is distributed primarily in different parts of the human brain (1, 2), and the cannabinoid-2 receptor (CB2R) has been detected primarily in cells of the peripheral immune system (3). The CB1R is of particular interest because its endogenous lipid ligands are involved in the regulation of energy metabolism and body weight, and in drug and substance addiction in animals and humans (4-6). The motivation to feed oneself was reported to be regulated by CB1R ligands in rats, and CB1R knockout mice were shown to be lean and resistant to dietary obesity (7, 8). Consequently, SR-141716A, a reverse agonist (i.e., it binds to the same site on the receptor as agonist, but mediates an opposite effect), is now available in the European Union for the treatment of obesity (9).

Investigators have been interested in the in vivo imaging of CB1R and have developed ligands that can be used in conjunction with single-photon emission computed tomography (SPECT) and positron emission tomography (PET). The agents developed so far to study the CB1R show high, non-specific binding (a characteristic of lipophilic compounds), have a low penetration of the brain (a characteristic of highly polar or lipophilic compounds), display a low affinity for the receptor, and produce unsatisfactory images (9-11). Although compounds labeled with radioactive carbon (^11^C) produced satisfactory results with PET, these compounds have a short half-life (20.4 min) (9, 12). In an effort to develop a PET ligand for CB1R with a longer half-life, N-[2-(3-cyanophenyl)-3-(4-(2-[^18^F]fluoroethoxy)phenyl)-1-methylpropyl]-2-(5-methyl-2-pyridyloxy)-2-methylpropanamide ([^18^F]MK-9470), a compound labeled with radioactive fluoride (^18^F), was developed and evaluated in baboons and humans (9, 13, 14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK9470+synthesis)]

A phenol precursor of [^18^F]MK-9470 was used to produce the radiochemical as described by Burns et al. (9). Briefly, Kryptofix222 was added to an aqueous solution of ^18^F, and the solution was dried under argon at 115°C. After cooling, a mixture of bromoethyltriflate in 1,2-dichlorobenzene was added to the mixture, and the solution was heated to 115°C. This was followed by a flow of argon to distill the [^18^F]fluoroethylbromide produced through a short ascarite column into a mixture of N-[2-(3-cyanophenyl)-3-(4-hydroxyphenyl)-1-methylpropyl]-2-(5-methyl-2-pyridyloxy)-2-methylpropanamide in dimethylformamide containing cesium carbonate (Cs_2_CO_3_) at room temperature. The mixture was subsequently transferred to a V-vial containing Cs_2_CO_3_ preheated to 100°C, and the solution was heated at this temperature for 5 min, diluted with water, and purified with reverse-phase high-performance liquid chromatography using a Waters RP C_18_ XTerra column. The appropriate fraction was concentrated and transferred under vacuum to another vial to obtain [^18^F]MK-9470. The radiochemical yield of the reaction was reported to be 3.1% with a purity of >98% and a specific activity of 116 TBq/mmol (1,359 Ci/mmol). For use in humans, the collected fractions were sterile-filtered and diluted to 6.0% ethanol in sodium acetate buffer (pH 5.5). These preparations were reported to be >95% pure and always had a specific activity >10 GBq/μmol (0.27 Ci/μmol). The stability of [^18^F]MK-9470 was not reported (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK9470+in+vitro)]

In vitro binding studies were performed as described by Patel et al. (15). The 50% inhibitory concentration of [^18^F]MK-9470 for humans was reported to be 0.7 nM (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK-9470+rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK-9470+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK-9470+nonhuman+primates)]

The biodistribution of [^18^F]MK-9470 was investigated in rhesus monkey brains (9). The animals (n = 4) were given a bolus intravenous (IV) injection of the radiochemical, and imaging was started at the time of injection. PET scans showed that [^18^F]MK-9470 accumulated primarily in gray matter regions of the monkey brain with significantly lower levels in the white matter. A chase study was also performed. The animals were given a bolus injection of unlabeled MK-9470 120 min after the [^18^F]MK-9470 injection. This was followed by a constant infusion of MK-0364, a structural analog of MK-9470, until steady-state plasma levels of ~1 μM were attained, and the scan was continued for 180 min after initial injection. Under these conditions a substantial decrease in binding of [^18^F]MK-9470 was observed in the gray matter, dropping to levels close to those observed in the white matter. The reversibility of MK-9470-CB1R binding was also investigated. The monkeys were injected with [^18^F]MK-9470 followed by administration of a bolus injection of unlabeled MK-9470 (9). This was reported to result in rapid washout of the label from the various gray matter regions of the monkey brain, indicating that the receptor binding of [^18^F]MK-9470 was reversible.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+MK-9470+humans)]

Burns et al. investigated the in vivo uptake of [^18^F]MK-9470 in the brains of four healthy human volunteers (9). The individuals were given a bolus injection of the radiochemical, and imaging was initiated immediately. The label was observed to accumulate in all the gray matter areas of the brain, and it remained constant for 120–360 min after administration. The maximum uptake was observed in the striatum, frontal cortex, and posterior cingulated regions of the brain. The cerebellum had an intermediate level of uptake, and the lowest uptake was observed in the thalamus and the hippocampus.

Burns et al. also studied the occupancy of CB1R in the human brain (9). A total of nine healthy individuals received an oral dose of either MK-0364 (the doses were 1, 4, and 7.5 mg for 2, 3, and 2 volunteers, respectively) or placebo (n = 2 subjects) once a day for 14 days. Baseline scans were obtained before treatment and ~24 h after the last dose of placebo or MK-0364. The subjects were given a slow, bolus IV injection of [^18^F]MK-9470, and imaging was performed. The measured CB1R occupancy values for the 1, 4, and 7.5 mg doses of MK-0364 in the brain were reported to be 11 ± 1%, 23 ± 7%, and 41 ± 12%, respectively (9).

The biodistribution and radiation dosimetry of [^18^F]MK-9470 was studied in healthy human volunteers (14). Eight nonobese individuals were given a bolus injection of [^18^F]MK-9470 and underwent whole-body PET/computed tomography scans for 6 h after the injection. Brain uptake of the radiopharmaceutical reached a plateau between 90 and 120 min after injection. Between 3.2% and 4.9% of the injected dose was detected in the brain. The radiochemical was reported to be excreted primarily through the hepatobiliary route. On average, the absorbed dose values for the gall bladder, upper large intestine, small intestine, and liver were 159, 98, 87, and 86 μGy/MBq, respectively. The mean effective dose was reported to be 22.8 ± 4.3 μSv/MBq (14).

In another study, the cerebral CB1R distribution and variation with age (volunteer age range, 18.5 to 68.7 years) and gender was investigated under in vivo conditions in 50 healthy volunteers (13). The [^18^F]MK-9470 was administered through a slow IV injection, and the individuals were subjected to PET scans for 120 min. An increased binding of [^18^F]MK-9470 with age was reported only for women (P < 0.05), and this was evident mainly in the basal ganglia, lateral temporal cortex, and the limbic system, primarily in the hippocampus. The [^18^F]MK-9470 binding was higher in men compared with women (P < 0.001) and was detected mainly in clusters of the limbic system and the cortico-striato-thalmic-cortical circuit.

## Supplemental Information

[Disclaimers]

## References

1 Iversen L. (2003). Cannabis and the brain. Brain.
2 Glass M., Dragunow M., Faull R.L. (1997). Cannabinoid receptors in the human brain: a detailed anatomical and quantitative autoradiographic study in the fetal, neonatal and adult human brain. Neuroscience.
3 Van Sickle M.D., Duncan M., Kingsley P.J., Mouihate A., Urbani P., Mackie K., Stella N., Makriyannis A., Piomelli D., Davison J.S., Marnett L.J., Di Marzo V., Pittman Q.J., Patel K.D., Sharkey K.A. (2005). Identification and functional characterization of brainstem cannabinoid CB2 receptors. Science.
4 Van Gaal L. (2007). Reducing cardiometabolic risk through selective antagonism of CB1 receptors. Clin Cornerstone.
5 Lupica C.R., Riegel A.C. (2005). Endocannabinoid release from midbrain dopamine neurons: a potential substrate for cannabinoid receptor antagonist treatment of addiction. Neuropharmacology.
6 Maldonado R., Valverde O., Berrendero F. (2006). Involvement of the endocannabinoid system in drug addiction. Trends Neurosci.
7 Williams C.M., Kirkham T.C. (2002). Observational analysis of feeding induced by Delta9-THC and anandamide. Physiol Behav.
8 Ravinet Trillou C., Delgorge C., Menet C., Arnone M., Soubrie P. (2004). CB1 cannabinoid receptor knockout in mice leads to leanness, resistance to diet-induced obesity and enhanced leptin sensitivity. Int J Obes Relat Metab Disord.
9 Burns H.D., Van Laere K., Sanabria-Bohorquez S., Hamill T.G., Bormans G., Eng W.S., Gibson R., Ryan C., Connolly B., Patel S., Krause S., Vanko A., Van Hecken A., Dupont P., De Lepeleire I., Rothenberg P., Stoch S.A., Cote J., Hagmann W.K., Jewell J.P., Lin L.S., Liu P., Goulet M.T., Gottesdiener K., Wagner J.A., de Hoon J., Mortelmans L., Fong T.M., Hargreaves R.J. (2007). [18F]MK-9470, a positron emission tomography (PET) tracer for in vivo human PET brain imaging of the cannabinoid-1 receptor. Proc Natl Acad Sci U S A.
10 Gatley S.J., Gifford A.N., Volkow N.D., Lan R., Makriyannis A. (1996). 123I-labeled AM251: a radioiodinated ligand which binds in vivo to mouse brain cannabinoid CB1 receptors. Eur J Pharmacol.
11 Berding G., Schneider U., Gielow P., Buchert R., Donnerstag F., Brandau W., Knapp W.H., Emrich H.M., Muller-Vahl K. (2006). Feasibility of central cannabinoid CB1 receptor imaging with [124I]AM281 PET demonstrated in a schizophrenic patient. Psychiatry Res.
12 Horti A.G., Fan H., Kuwabara H., Hilton J., Ravert H.T., Holt D.P., Alexander M., Kumar A., Rahmim A., Scheffel U., Wong D.F., Dannals R.F. (2006). 11C-JHU75528: a radiotracer for PET imaging of CB1 cannabinoid receptors. J Nucl Med.
13 Van Laere K., Goffin K., Casteels C., Dupont P., Mortelmans L., de Hoon J., Bormans G. (2008). Gender-dependent increases with healthy aging of the human cerebral cannabinoid-type 1 receptor binding using [(18)F]MK-9470 PET. Neuroimage.
14 Van Laere K., Koole M., Sanabria Bohorquez S.M., Goffin K., Guenther I., Belanger M.J., Cote J., Rothenberg P., De Lepeleire I., Grachev I.D., Hargreaves R.J., Bormans G., Burns H.D. (2008). Whole-Body Biodistribution and Radiation Dosimetry of the Human Cannabinoid Type-1 Receptor Ligand 18F-MK-9470 in Healthy Subjects. J Nucl Med.
15 Patel S., Hamill T., Hostetler E., Burns H.D., Gibson R.E. (2003). An in vitro assay for predicting successful imaging radiotracers. Mol Imaging Biol.